# 2-[4-(4-[^18^F]Fluorobutyl)benzylsulfanyl]-3-methylchromene-4-one

Chemical name: | 2-[4-(4-[^18^F]Fluorobutyl)benzylsulfanyl]-3-methylchromene-4-one
Abbreviated name: | [^18^F]10
Synonym:
Backbone: | Compound
Target: | Mitochondrial complex I (MCI)
Mechanism: | Enzyme inhibitor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=methylchromene)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations that are rapidly taken up into cells in response to metabolic demand and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography (SPECT) agents and as tumor imaging agents. However, the high accumulation of Tc tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach to evaluating myocardial blood flow by use of positron-emitting radionuclides (e.g., ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibited short physical half-lives (<20 min). Lipophilic cations like [^11^C]triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MCI) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which 7 are encoded by mitochondrial DNA (7). MCI catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thereby the energy supply of the cell. It may also play direct roles in the mitochondrial permeability transition and cell death pathways. Myocardium has a high mitochondrial content because of high energy usage. 2-[4-(4-Fluorobutyl)benzylsulfanyl]-3-methylchromene-4-one (compound 10) is a potent MCI inhibitor with a hydrophobic heterocyclic chromone core (8). 2-[4-(4-[^18^F]Fluorobutyl)benzylsulfanyl]-3-methylchromene-4-one ([^18^F]10) has been synthesized for use in studies as a myocardium imaging PET agent.

### Related Resource Links:

- Chapters in MICAD (MCI (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D))
- Gene information in NCBI (MCI (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MCI (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=252010))
- Clinical trials (MCI (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+I+))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=methylchromene+synthesis)]

[^18^F]10 was prepared as described by Radeke et al. (8). [^18^F]KF/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor were heated in acetonitrile at 90°C for 30 min, followed by high-performance liquid chromatography purification. Average radiochemical yield was 6% with a total synthesis time of 90 min. Radiochemical purity was >99% with specific activities of 27.8–74.0 TBq/µmol (750–2,000 Ci/mmol) at end of synthesis. [^18^F]10 has a clog D_7.4_ value of 5.6.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20methylchromene%20and%20in%20vitro)]

Radeke et al. (8) reported that compound 10 inhibited NADH oxidation by bovine heart submitochondrial particles with a 50% inhibitory concentration value of 9 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20methylchromene%20and%20rodentia)]

Radeke et al. (8) performed biodistribution and PET imaging studies of [^18^F]10 in rats. [^18^F]10 accumulated mainly in the heart (2.24 ± 0.27% injected dose (ID/g)), kidney (2.00 ± 0.31% ID/g), and liver (1.93 ± 0.14% ID/g), with low blood (0.11 ± 0.02% ID/g) and brain radioactivity (~0.26% ID/g) at 30 min after injection. Retention of [^18^F]10 in the heart was good in that 66% of the radioactivity at 30 min was present at 120 min, whereas retention was much less in the other organs with the exception of the femur. The uptake in the femur was 0.36 ± 0.04% ID/g at 30 min and 0.74 ± 0.06% ID/g at 120 min, indicating some defluorination of [^18^F]10. PET imaging showed that [^18^F]10 accumulated mainly in the heart, followed by the kidney and liver, with low accumulation in the lung. Good myocardial images were observed at 25–35 min after injection, and complete images were observed at 55–60 min with little interference from the lung. Bone uptake was observed in images after 30 min. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=methylchromene+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20methylchromene%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20methylchromene%20and%20human)]

No publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Radeke H., Hanson K., Yalamanchili P., Hayes M., Zhang Z.Q., Azure M., Yu M., Guaraldi M., Kagan M., Robinson S., Casebier D. (2007). Synthesis and biological evaluation of the mitochondrial complex 1 inhibitor 2-[4-(4-fluorobutyl)benzylsulfanyl]-3-methylchromene-4-one as a potential cardiac positron emission tomography tracer. J Med Chem.